# ^64^Cu-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-quantum dot-c(Arg-Gly-Asp-D-Tyr-Lys)

Chemical name: | ^64^Cu-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-quantum dot-c(Arg-Gly-Asp-D-Tyr-Lys)
Abbreviated name: | ^64^Cu-DOTA-QD-RGD, ^64^Cu-DOTA-QD-c(RGDyK)
Synonym:
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor-ligand binding
Method of detection: | Positron emission tomography (PET); optical, near-infrared (NIR) fluorescence
Source of signal: | ^64^Cu and quantum dot
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Quantum+dot+Cu+RGD)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low fluorescence background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence (NIRF) imaging is becoming a non-invasive alternative to radionuclide imaging in small animals (4, 5).

Fluorescent semiconductor quantum dots (QDs) are nanocrystals made of CdSe/CdTe-ZnS with radii of 1–10 nm (6-8). They can be tuned to emit light in a range of wavelengths by changing their sizes and composition, thus providing broad excitation profiles and high absorption coefficients. They have narrow and symmetric emission spectra with long excited-state lifetimes (20–50 ns) compared with fluorescent dyes (1–10 ns). QDs possess good quantum yields of 40–90% and high extinction coefficients, and they are more photo-stable than conventional organic dyes. They can be coated and capped with hydrophilic materials for additional conjugations with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds, which are tested in vitro and in vivo (8-12). Although many cells have been labeled with QDs in vitro with little cytotoxicity, there are only limited studies of long-term toxicity of QDs in small animals (13-21), and little is known about the toxicity and the mechanisms of clearance and metabolism of QDs in humans.

Integrins are a family of heterodimeric, cell-surface glycoproteins that mediate diverse biological events involving cell–cell and cell–matrix interactions (22). Integrins comprise an α and a β subunit, and they are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor class, affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (23-28). The α_v_β_3_ integrin is strongly expressed on tumor cells and activated endothelial cells. In contrast, expression of α_v_β_3_ integrin is weak on resting endothelial cells and on most normal tissues. The α_v_β_3_ antagonists are being studied as anti-tumor and anti-angiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (27, 29, 30). A tripeptide sequence comprising Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins including α_v_β_3_. Various radiolabeled cyclic RGD peptides have been introduced for tumor imaging and tumor angiogenesis (31). The multimodality probe ^64^Cu-DOTA-QD-c(RGDyK) has been developed for PET and NIRF imaging of tumor vasculature to study in vivo biodistribution of the tracer in tumor-bearing mice (32). ^64^Cu-DOTA-QD-c(RGDyK) has been shown to have a high accumulation in the tumor vasculature with little extravasation and a predominant liver and spleen accumulation.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Quantum+dot+Cu+RGD+synthesis)]

Commercially available QDs within amine-functionalized groups (emission, 705 nm; QD705, Invitrogen) were mixed with c(RGDyK)-4-maleimidobutyric acid N-hydroxysuccinimide ester and DOTA-N-hydroxysulfosuccinimide ester at room temperature for 1 h (32). The resulting DOTA-QD-RGD was purified with column chromatography. DOTA-QD was also prepared as a control. The molar ratio of DOTA to QD was estimated to be 28.2 for DOTA-QD-RGD and 118 for DOTA-QD. The number of RGD peptides was estimated to be 90 per QD nanoparticle. DOTA-QD-RGD or DOTA-QD (50 µg) was added to 74 MBq (2 mCi) of ^64^CuCl_2_ in sodium acetate buffer (pH 6.5). The reaction mixture was incubated at 40°C for 1 h. The ^64^Cu-labeling yield was >90% for both QD conjugates (n = 3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Quantum+dot+Cu+RGD+in%20vitro)]

Cai et al. (32) performed competitive cell-binding assays using human glioblastoma U87MG tumor cells (expressing α_v_β_3_). DOTA-QD-RGD inhibited the binding of ^125^I-echistatin in a dose-dependent manner with a 50% inhibition concentration value of 3.88 nM, which was ~60-fold higher than c(RGDyK). Fluorescence microscopy showed that DOTA-QD had minimal binding to U87MG cells, whereas DOTA-QD-RGD (1 nM) bound to the cell surface of U87MG cells. The DOTA-QD-RGD binding was inhibited by 1,000 nM c(RGDyK). On the other hand, DOTA-QD-RGD did not bind to α_v_β_3_-negative C6 cells.

## Animal Studies

### Rodents

[PubMed]

Cai et al. (32) used a whole-body PET imaging system at 1, 5, 18, and 25 h to study the accumulation of ^64^Cu-DOTA-QD-c(RGDyK) in mice bearing U87MG tumors. ^64^Cu-DOTA-QD-c(RGDyK) (0.02 nmol/mouse) injected intravenously into nude mice (n = 3/group) bearing U87MG tumors (maximal tumor/muscle ratio = 4.1) showed that the liver, spleen, and lymph nodes were clearly visualized. Tumor accumulation of ^64^Cu-DOTA-QD-c(RGDyK) was ~1% injected dose/gram (ID/g) at 1 h, 2.2% ID/g at 5 h, 4.0% ID/g at 18 h, and 4.3% ID/g at 25 h, distinctly higher than ^64^Cu-DOTA-QD (<1% ID/g) at all time points. There was a marked intensity of signal in the liver (~50% ID/g) for both conjugates. Ex vivo PET imaging and NIRF imaging scans were performed on tissues harvested at 5 h. The liver, spleen, and bone marrow all had very strong signals, and the U87MG tumor exhibited significantly higher uptake than the heart, kidneys, and muscle. Both in vivo and ex vivo PET imaging data produced similar tissue/muscle ratios. The liver/muscle, spleen/muscle, bone/muscle, and kidney/muscle ratios were ~100:1, 30:1, 10:1, and 2:1, respectively. The U87MG tumor/muscle ratios for DOTA-QD-RGD and DOTA-QD were ~4:1 and 1:1, respectively. The liver/muscle, spleen/muscle, bone/muscle, kidney/muscle, and tumor/muscle ratios for NIRF imaging were ~100:1, 50:1, 40:1, 1:1, and 2:1, respectively. No blocking experiments were performed. Excellent linear correlation was observed between the signals measured with in vivo PET imaging and those measured with ex vivo NIRF imaging and tissue homogenate fluorescence (r^2^ = 0.93). Histological examination of the tumor sections revealed that DOTA-QD-RGD targets primarily the tumor vasculature through an RGD–integrin α_v_β_3_ interaction on the endothelial cells, with little extravasation.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Quantum+dot+Cu+RGD+and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Quantum+dot+Cu+RGD+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed]

No publication is currently available.

## NIH Support

R21 EB001785, R21 R01 CA119053, R21 CA121842, R21 CA102123, P50 CA114747, U54 CA119367, R24 CA93862

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Robeson W., Dhawan V., Belakhlef A., Ma Y., Pillai V., Chaly T., Margouleff C., Bjelke D., Eidelberg D. (2003). Dosimetry of the dopamine transporter radioligand 18F-FPCIT in human subjects. J Nucl Med.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Zheng G., Li H., Yang K., Blessington D., Licha K., Lund-Katz S., Chance B., Glickson J.D. (2002). Tricarbocyanine cholesteryl laurates labeled LDL: new near infrared fluorescent probes (NIRFs) for monitoring tumors and gene therapy of familial hypercholesterolemia. Bioorg Med Chem Lett.
7 Gao X., Nie S. (2005). Quantum dot-encoded beads. Methods Mol Biol.
8 Pinaud F., Michalet X., Bentolila L.A., Tsay J.M., Doose S., Li J.J., Iyer G., Weiss S. (2006). Advances in fluorescence imaging with quantum dot bio-probes. Biomaterials.
9 Alivisatos A.P., Gu W., Larabell C. (2005). Quantum dots as cellular probes. Annu Rev Biomed Eng.
10 Hilger I., Leistner Y., Berndt A., Fritsche C., Haas K.M., Kosmehl H., Kaiser W.A. (2004). Near-infrared fluorescence imaging of HER-2 protein over-expression in tumour cells. Eur Radiol.
11 Medintz I.L., Uyeda H.T., Goldman E.R., Mattoussi H. (2005). Quantum dot bioconjugates for imaging, labelling and sensing. Nat Mater.
12 Kabas J.S., Kisslo J., Flick C.L., Johnson S.H., Craig D.M., Stanley T.E., Smith P.K. (1990). Intraoperative perfusion contrast echocardiography. Initial experience during coronary artery bypass grafting. J Thorac Cardiovasc Surg.
13 Akerman M.E., Chan W.C., Laakkonen P., Bhatia S.N., Ruoslahti E. (2002). Nanocrystal targeting in vivo. Proc Natl Acad Sci U S A.
14 Braydich-Stolle L., Hussain S., Schlager J.J., Hofmann M.C. (2005). In vitro cytotoxicity of nanoparticles in mammalian germline stem cells. Toxicol Sci.
15 Kim S., Lim Y.T., Soltesz E.G., De Grand A.M., Lee J., Nakayama A., Parker J.A., Mihaljevic T., Laurence R.G., Dor D.M., Cohn L.H., Bawendi M.G., Frangioni J.V. (2004). Near-infrared fluorescent type II quantum dots for sentinel lymph node mapping. Nat Biotechnol.
16 Gao X., Cui Y., Levenson R.M., Chung L.W., Nie S. (2004). In vivo cancer targeting and imaging with semiconductor quantum dots. Nat Biotechnol.
17 Han M., Gao X., Su J.Z., Nie S. (2001). Quantum-dot-tagged microbeads for multiplexed optical coding of biomolecules. Nat Biotechnol.
18 Lovric J., Bazzi H.S., Cuie Y., Fortin G.R., Winnik F.M., Maysinger D. (2005). Differences in subcellular distribution and toxicity of green and red emitting CdTe quantum dots. J Mol Med.
19 Ohnishi S., Lomnes S.J., Laurence R.G., Gogbashian A., Mariani G., Frangioni J.V. (2005). Organic alternatives to quantum dots for intraoperative near-infrared fluorescent sentinel lymph node mapping. Mol Imaging.
20 Shiohara A., Hoshino A., Hanaki K., Suzuki K., Yamamoto K. (2004). On the cyto-toxicity caused by quantum dots. Microbiol Immunol.
21 Soltesz E.G., Kim S., Laurence R.G., DeGrand A.M., Parungo C.P., Dor D.M., Cohn L.H., Bawendi M.G., Frangioni J.V., Mihaljevic T. (2005). Intraoperative sentinel lymph node mapping of the lung using near-infrared fluorescent quantum dots. Ann Thorac Surg.
22 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
23 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
24 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
25 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
26 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
27 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
28 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
29 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
30 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
31 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
32 Cai W., Chen K., Li Z.B., Gambhir S.S., Chen X. (2007). Dual-function probe for PET and near-infrared fluorescence imaging of tumor vasculature. J Nucl Med.